# (+)-8-Chloro-5-(7-benzofuranyl)-7-hydroxy-3-[^11^C]methyl-2,3,4,5-tetrahydro-1H-3-benzazepine

Chemical name: | (+)-8-Chloro-5-(7-benzofuranyl)-7-hydroxy-3-[^11^C]methyl-2,3,4,5-tetrahydro-1H-3-benzazepine
Abbreviated name:
Synonym: | [^11^C]NNC 112
Backbone: | Compound
Target: | D_1_ dopamine receptors
Mechanism: | Receptor binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20NNC%20112)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition, and emotion (2, 3). Dopamine receptors are involved in the pathophysiology of neuropsychiatric diseases such as Parkinson’s disease, Alzheimer's disease, Huntington’s disease, and schizophrenia (4). Five subtypes of dopamine receptors, D_1_ through D_5_, have been well characterized pharmacologically and biochemically (5). These five subtypes are classified into two subfamilies: D_1_-like (D_1_ and D_5_) and D_2_-like (D_2_, D_3_, and D_4_) dopamine receptors. D_1_-like and D_2_-like receptors exert synergistic as well as opposite effects at both the biochemical and overall system level. A great majority of striatal D_1_ and D_2_ receptors are localized postsynaptically on caudate-putamen neurons and to a lesser extent presynaptically on nigrostriatal axons.

(R)-(+)-8-Chloro-2,3,4,5-tetrahydro-3-[^11^C]methyl-5-phenyl-1H-3-benzazepin-7-ol ([^11^C]SCH 23390) was the first positron emission tomography (PET) radioligand for D_1_ receptor studies. However, [^11^C]SCH 23390 exhibits a low neocortex/cerebellum ratio (1.5), which makes it difficult to estimate the D_1_ receptor density in the neocortex. (+)-8-Chloro-5-(7-benzofuranyl)-7-hydroxy-3-[^11^C]methyl-2,3,4,5-tetrahydro-1H-3-benzazepine ([^11^C]NNC 112) was also found to be a selective, high-affinity antagonist of D_1_ receptors, but to have only a marginal effect on D_2_, α_1_-adrenergic, muscarinic, and histaminergic receptors and only a slight effect on 5-HT_2_ receptors (6, 7). [^11^C]NNC 112 was found to display higher specific signal/noise ratios than [^11^C]SCH 23390. [^11^C]NNC 112 PET has been developed to study D_1_ receptor occupancy and density in the striatum and neocortex in humans.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20NNC%20112%20and%20synthesis)]

[^11^C]NNC 112 was synthesized by alkylation of the desmethyl compound with [^11^C]methyl triflate (8). Reaction in acetone with subsequent chromatographic separation gave radiochemical yields of 50-60%, with a total synthesis time of 25-30 min and a radiochemical purity >99%. The average specific activity was 111 GBq/μmol (3 Ci/μmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20NNC%20112%20and%20in%20vitro)]

NNC 112 has been reported to have selective binding affinity to D_1_ (striatum) and 5-HT_2_ (frontal cortex) receptor sites in homogenates of rat brain membranes (6, 7). The K_i_ values for D_1_, D_2_, and 5-HT_2_ were 0.18, 898, and 18 nM, respectively. The affinity for the D_2_ receptor is about 4,900-fold lower than that for the D_1_ receptor. NNC 112 has a 50% inhibitory concentration (IC_50_) of 2,300 nM for the α_1_-adrenergic receptor. The affinity for the 5-HT_2_ receptor is about 100-fold lower than that for the D_1_ receptor, suggesting that specific [^11^C]NNC 112 binding visualized by PET represents mainly binding to D_1_ receptors. Farde and Hall (9) reported that the receptor densities of D_1_ to D_2_ in the human putamen-caudate regions are similar and that there are more D_1_ receptors than D_2_ receptors in various cortical regions.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20NNC%20112%20and%20rodentia)]

Biodistribution studies in rat brain showed high accumulation of radioactivity in the striatum (2.05 ± 0.43% injected dose (ID)/g), followed by the prefrontal cortex (0.52 ± 0.10% ID/g), hippocampus (0.41 ± 0.09% ID/g), and cerebellum (0.19 ± 0.04% ID/g) at 30 min after injection of [^11^C]NNC 112 (10). The striatum/cerebellum ratio was 10.79.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20NNC%20112%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

Using PET, Rosa-Neto et al. (11) directly compared the distributions of dopamine D_1_ and D_2/3_ receptors in six Gottingen minipigs. The binding potentials (BPs) of [^11^C]NNC 112 for dopamine D_1_ receptors and [^11^C]raclopride for dopamine D_2/3_ receptors were calculated in pig striatum by use of metabolite-corrected arterial inputs or with cerebellum used as the reference region. Depending on the method for quantitation, the BP for [^11^C]NNC 112 was 1.2-5.1 in pig striatum, whereas the BP for [^11^C]raclopride was 1.0-1.8. The reference tissue method of Logan provided the most stable estimate of BP for [^11^C]NNC 112. Dopamine D_1_ binding was relatively more abundant in the ventral-anterior striatum of the pig, whereas dopamine D_2/3_ binding was greater in the dorsal-posterior striatum. Similar comparisons were made for the BPs of [^11^C]SCH 23390 for dopamine D_1_ receptors and for [^11^C]raclopride in the brains of six rhesus monkeys. The fraction of unchanged [^11^C]NNC 112 in plasma was 45, 24, and 3% at 5, 10, and 60 min, respectively.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20NNC%20112%20and%20%28primate%20not%20human%29)]

Halldin et al. (8) performed PET studies in the brains of cynomolgus monkeys and found high accumulation of radioactivity in the brain (4.2% ID) with higher accumulation in the striatum than in the cerebellum at 4 min after injection of 37 MBq (1 mCi) of [^11^C]NNC 112. The striatum/cerebellum and neocortex/cerebellum ratios were 5.77 ± 0.31 and 2.36 ± 0.14 at 40-50 min after injection, respectively. Inhibition by the specific D_1_ receptor antagonist SCH 23390 (2.5 mg/kg 21-23 min after [^11^C]NNC 112 injection) was 80% in the striatum and neocortex at 72 min after injection. However, the 5-HT_2_ antagonist ketanserin (2 mg/kg before or after [^11^C]NNC 112 injection) showed no inhibition, indicating that binding of [^11^C]NNC 112 to D_1_ receptors in the brain is specific and reversible.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20NNC%20112%20and%20human)]

In a PET study of D_1_ receptor distribution in human brain, Halldin et al. (8) reported that [^11^C]NNC 112 showed major localization of radioactivity in the striatum and neocortex. The striatum/cerebellum and neocortex/cerebellum ratios were 3.8 and 1.8, respectively. Transient equilibrium was achieved at 40-50 min after injection. Linear graphical analysis gave of distribution volumes for the putamen, frontal cortex, and cerebellum of 15.2, 5.8, and 3.9, respectively. The fraction of unchanged [^11^C]NNC 112 in plasma was 50% and 18% at 10 and 30 min, respectively.

Abi-Dargham et al. (12) studied 6 healthy volunteers, using kinetic and Logan graphical analysis to estimate four parameters with good reproducibility and good agreement. However, there was noise-dependent bias in the graphical but not in the kinetic analysis. Another PET study by Abi-Dargham et al. (13) in 16 patients with schizophrenia (no psychotropic medication at least 14 days before the study) and in 16 normal subjects revealed that the BP of [^11^C]NNC 112 was significantly elevated in the dorsolateral prefrontal cortex (DLPFC) of patients with schizophrenia (1.63 ± 0.39 ml/g) compared with the controls (1.27 ± 0.44 ml/g).

Narendran et al. (14) compared regional brain BPs of [^11^C]NNC 112 in 14 chronic ketamine users and 14 normal volunteers. There was a significant increase in [^11^C]NNC 112 BP in the DLPFC of ketamine users (1.68 ± 0.40 ml/g) compared with controls (1.35 ± 0.35 ml/g). No significant differences were observed in other cortical, limbic, or striatal regions. Slifstein et al. (15) reported that specific binding of [^11^C]NNC 112 in the brain cortical regions was reduced by 20-30% after administration of 2 mg of risperidone to inhibit serotonin 5-HT_2A_ receptors in 7 healthy subjects. No inhibition was observed in the striatum. These results suggested that there are ~5-10 fold selectivity of [^11^C]NNC 112 for D1 versus 5-HT_2A_ receptors.

Cropley et al. (16) reported on PET scans in 7 healthy volunteers after injection of ~710 MBq (19 mCi) of [^11^C]NNC 112. Absorbed doses were found to be 32.4 μGy/MBq (0.12 rad/mCi) for the gallbladder, 22.2 μGy/MBq (0.082 rad/mCi) for the liver, 16.9 μGy/MBq (0.063 rad/mCi) for the lungs, 16.6 μGy/MBq (0.061 rad/mCi) for the kidneys, 15.7 μGy/MBq (0.058 rad/mCi) for the urinary bladder wall, 9.4 μGy/MBq (0.035 rad/mCi) for the spleen, and 6.9 μGy/MBq (0.026 rad/mCi) for the brain. The effective dose was 5.7 μSv/MBq (21.1mrem/mCi).

## Supplemental Information

[Disclaimers (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=disclaimer)]

Chemistry

Synthesis Protocol

Toxicology

## NIH Support

Intramural research program, R01 MH59144-01, MH661710-03, K02 MH01603-0

## References

1 Slavicek J.M., Hayes-Plazolles N. (2003). The Lymantria dispar nucleopolyhedrovirus contains the capsid-associated p24 protein gene. Virus Genes.
2 Carbon M., et al. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
3 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
4 Seeman P., et al. (1987). Human brain D1 and D2 dopamine receptors in schizophrenia, Alzheimer's, Parkinson's, and Huntington's diseases. Neuropsychopharmacology.
5 Stoof J.C., Kebabian J.W. (1984). Two dopamine receptors: biochemistry, physiology and pharmacology. Life Sci.
6 Andersen P.H., et al. (1992). NNC-112, NNC-687 and NNC-756, new selective and highly potent dopamine D1 receptor antagonists. Eur J Pharmacol.
7 Nielsen E.B., Andersen P.H. (1992). Dopamine receptor occupancy in vivo: behavioral correlates using NNC-112, NNC-687 and NNC-756, new selective dopamine D1 receptor antagonists. Eur J Pharmacol.
8 Halldin C., et al. (1998). Carbon-11-NNC 112: a radioligand for PET examination of striatal and neocortical D1-dopamine receptors. J Nucl Med.
9 Farde L., Hall H. (1992). Positron emission tomography--examination of chemical transmission in the living human brain. Development of radioligands. Arzneimittelforschung.
10 Guo N., et al. (2003). Dopamine depletion and in vivo binding of PET D1 receptor radioligands: implications for imaging studies in schizophrenia. Neuropsychopharmacology.
11 Rosa-Neto P., Doudet D.J., Cumming P. (2004). Gradients of dopamine D1- and D2/3-binding sites in the basal ganglia of pig and monkey measured by PET. Neuroimage.
12 Abi-Dargham A., et al. (2000). Measurement of striatal and extrastriatal dopamine D1 receptor binding potential with [11C]NNC 112 in humans: validation and reproducibility. J Cereb Blood Flow Metab.
13 Abi-Dargham A., et al. (2002). Prefrontal dopamine D1 receptors and working memory in schizophrenia. J Neurosci.
14 Narendran R., et al. (2005). Altered prefrontal dopaminergic function in chronic recreational ketamine users. Am J Psychiatry.
15 Slifstein M., et al. (2007). [11C]NNC 112 selectivity for dopamine D1 and serotonin 5-HT(2A) receptors: a PET study in healthy human subjects. J Cereb Blood Flow Metab.
16 Cropley V.L., et al. (2006). Whole-Body Biodistribution and Estimation of Radiation-Absorbed Doses of the Dopamine D1 Receptor Radioligand 11C-NNC 112 in Humans. J Nucl Med.